# L36-Cy5 anti-laminin trimerbody

Chemical name: | L36-Cy5 anti-laminin trimerbody
Abbreviated name:
Synonym:
Agent Category: | Antibody
Target: | Laminin
Target Category: | Antigen
Method of detection: | Near-infrared fluorescence (NIR) imaging
Source of signal / contrast: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20tumor%20AND%20imaging)]

The laminin family of glycoproteins is a major constituent of both epithelial and vascular basement membranes (BMs) (1, 2). L36-Cy5 anti-laminin trimerbody is an anti-laminin single-chain variable fragment (scFv) trimerbody labeled with the fluorescent reporter Cy5, and it has been developed for optical imaging of solid tumors (3, 4).

Monoclonal antibodies (mAbs) and antibody fragments have been used for tumor targeting for many years. An ideal tumor-targeting antibody should fulfill several requirements: rapid tissue penetration, high target retention, and rapid blood clearance (5, 6). The format and molecular weight of an antibody are critical factors that influence its pharmacokinetics and in vivo efficacy (5-7). Intact mAbs (~150 kDa) display low blood clearance and incomplete tumor penetration. The production yield of mAbs is limited (5). These disadvantages of mAbs are partially overcome by developing recombinant scFv antibody fragments. Monovalent scFv (25–30 kDa) represents the smallest functional component of an antibody, and it is more efficient in tumor penetration. However, the scFv fragment is cleared from blood too rapidly, and it has poor binding affinity and tumor retention. Bivalent antibodies such as diabodies (55–60 kDa) and minibodies (~80 kDa) possess more ideal tumor-targeting characteristics such as compact size and higher binding affinity than monovalent scFv (6). Diabodies are dimeric molecules consisting of two scFv fragments connected with a short linker. Minibodies are formed by the fusion of scFv fragments with the IgG1 CH3 domain. Improved affinity of the bivalent antibodies relies on binding and rebinding, as well as simultaneous binding to different molecules of the antigen (3, 4). An issue is that it will lead to small gains in functional affinity if simultaneous multiple binding is not sterically possible. Taking the advantages of collagen XVIII NC1 domain and scFv fragments, Sanchez-Arévalo Lobo et al. developed a multivalent antibody, termed “trimerbody,” for in vivo tumor targeting (4). The NC1 domain of collagen XVIII consists of three functionally different subdomains: an N-terminal noncovalent trimerization subdomain implicated in self-assembly of homotrimers, a central protease-sensitive hinge region, and a compact C-terminal endostatin globular subdomain (3, 4, 8). The trimerbody is designed and constructed by connecting scFv fragments to the N-terminal trimerization subdomains of NC1 through flexible linkers. The resulting trimerbody has a tripod-shaped structure with three scFv heads oriented radially outward. The artificial linker between the N-terminal scFv and NC1 domain consisted of 21 amino acids. The maximal length of the linker is 79.8 Å if the conformation is fully extended, which allows the scFv heads to be highly flexible and provides numerous binding geometries (3, 4).

Based on the concept of trimerbody design, Cuesta et al. constructed a fluorescently labeled L36-Cy5 anti-laminin trimerbody (3). The laminin family (15 members and 12 known chain genes to date) plays an important role in cell adhesion, migration, and angiogenesis (1, 9). Laminins interact with endothelial cells through integrin or non-integrin receptor families and modulate their behavior during angiogenesis (10, 11). Knockout of laminin-8 α4 chain is characterized by abnormal blood vessel maturation (11). Deregulation of the cell–laminin interactions is associated with tumor invasion (2, 12). Several laminin members are highly expressed in the tumor blood vessels (13). A switch from β2-containing to β1-containing vascular laminins has been found during the progression of breast and brain tumors, which may constitute a general feature of vascular BM changes in solid tumors (13, 14). The β1 chains of laminin-2, laminin-8, and laminin-10 have been detected in newly formed tumor vessels and are considered to be a potential target for antiangiogenic therapy (13, 15). Sanchez-Arévalo Lobo et al. demonstrated that blocking the cell binding sites of laminins with anti-laminin monovalent scFv fragment (L36) or trimerbody inhibited the tumor angiogenesis and growth in vivo (4). The epitope recognized by L36 is located in a highly flexible area in the middle part of the triple coiled-coil laminin domain, which interacts with the α_2_β_1_ integrin on the endothelial cell surface (16). With optical imaging, Cuesta et al. further demonstrated that the L36-Cy5 anti-laminin trimerbody was well localized in both fibrosarcomas and adenocarcinomas after systemic administration to the mice bearing the tumor xenografts (3).

Based on the same design concept, the trimerbody targeting the carcinoembryonic antigen (CEA) MFE23-Cy5 anti-CEA trimerbody (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html) was also constructed and analyzed for its feasibility in imaging CEA-positive tumors (3).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

The synthesis of the L36-Cy5 anti-laminin trimerbody and B1.8-Cy5 anti-hapten 4-hydroxy-5-iodo-3-nitrophenyl (anti-NIP) trimerbody (used as control) was described in detail by Cuesta et al. and Sanchez-Arévalo Lobo et al., separately (3, 4). Briefly, the NC1 sequence was first amplified from the mouse α1(XVIII) clone mc3b and ligated into the plasmid pCR3.1-L36 (containing the L36 scFv antibody gene) to obtain the plasmid pCR3.1-L36-NC1^ES+^. A flexible linker was then ligated into the pCR3.1-L36-NC1^ES+^, resulting in pCR3.1-L36-linker-NC1^ES+^. To construct the expression plasmid pCR3.1-L36-NC1^ES-^, a plasmid pCR3.1-NC1 was first constructed by removing the ClaI-BglII fragment from the plasmid pCR3.1-L36-linker-NC1^ES+^, and by inserting an oligonucleotide containing an NruI site. The NC1 trimerization subdomain was then amplified from the plasmid pCR3.1-NC1 and ligated into the backbone of plasmid pCR3.1-L36, to obtain the pCR3.1-L36-NC1^ES-^. To construct the B1.8 anti-NIP trimerbody expression plasmid, the NC1 trimerization subdomain (a 252-bp fragment) was generated from the plasmid pCR3.1-L36-NC1^ES-^ and then ligated into the plasmid pCEP4-B1.8, resulting in the expression plasmid pCEP4-B1.8-NC1^ES-^. The plasmid pCEP4-B1.8 contains the B1.8 scFv gene and the polyhistidine and c-myc epitopes. To express the trimerbodies, HEK-293 (human embryo kidney epithelia) cells were transfected with the expression plasmids pCR3.1-L36-NC1^ES-^ and pCEP4-B1.8-NC1^ES-^, separately. Stably transfected HEK-293 cell lines were established through G418 or hygromycin B selection. The trimerbodies were isolated in a functionally active form from the serum-free conditioned medium of the transfected HEK-293 cells, and they were purified with immobilized metal affinity chromatography. Purified trimerbodies were labeled with Cy5 N-hydroxysuccinimide esters. The labeling ratio of Cy5/trimerbody was close to 1:1. The purity of the yielded trimerbodies was >95%. The trimeric nature of the trimerbodies was confirmed with ultracentrifugation and analytical gel filtration chromatography. The estimated molecular weight of L36 anti-laminin trimerbody was 109.3 kDa (the theoretical mass of the trimer was 111.4 kDa).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

Cuesta et al. first analyzed the stability of L36 anti-laminin trimerbody by incubation of the trimerbody with mouse and human serum at 37°C for various lengths of time (3). Their data showed that L36 anti-laminin trimerbody retained 80–90% of its binding activity after 72 h of incubation. They then investigated the functionality of the trimerbodies against plastic immobilized NIP-BSA conjugates (NIP_10_-BSA) and murine laminin with ELISA. Both the anti-laminin and anti-NIP trimerbodies specifically recognized the respective immobilized antigens. The anti-NIP trimerbody had at least a 100-fold increase in functional affinity to NIP_10_-BSA antigen compared to its monovalent counterpart (4). Surface plasmon resonance analysis further demonstrated that the anti-NIP trimerbody had a slower dissociation than the monomeric anti-NIP scFv, consistent with multivalent binding to the antigen molecules. The detailed binding affinity data of the L36-Cy5 anti-laminin trimerbody were not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=laminin%20AND%20trimerbody)]

The potential of the L36-Cy5 anti-laminin trimerbody for in vivo tumor imaging was assessed in nude mice bearing human tumor xenografts (3). MKN45 (human stomach adenocarcinoma), HT1080 (human fibrosarcoma), or HeLa (human cervical adenocarcinoma) cells were implanted subcutaneously into the dorsal space of 6-week-old female Hsd:athymic nude-Foxn1^nu^ mice (n = 4/group). Mice were injected with 100 µl of the trimerbody in phosphate-buffered saline (5 mg/kg) through the tail vein. Whole-body fluorescence imaging showed that both anti-laminin and anti-NIP trimerbodies had a rapid renal clearance after intravenous injection, with peak signal intensity at 3 h, and no detectable signal in the bladder at 48 h after injection. Elimination of the L36-Cy5 monovalent scFv (with half-lives <15 min) was more rapid than the trimerbody, and the fluorescence was undetectable in the bladder at 24 h after injection. The L36-Cy5 anti-laminin trimerbody showed localization in all the tumors studied, regardless of tumor type. The maximum tumor uptake was observed at 24 h after injection. The L36-Cy5 monovalent scFv also showed specific tumor accumulation, but at a much lower level than that of the L36-Cy5 trimerbody. The control B1.8-Cy5 anti-NIP trimerbody showed no detectable localization in any of the three tumor types. The detailed biodistribution of the L36-Cy5 anti-laminin trimerbody in blood and other organs was not reported. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Miner J.H. (2008). Laminins and their roles in mammals. Microsc Res Tech.
2 Givant-Horwitz V., Davidson B., Reich R. (2005). Laminin-induced signaling in tumor cells. Cancer Lett.
3 Cuesta A.M., Sanchez-Martin D., Sanz L., Bonet J., Compte M., Kremer L., Blanco F.J., Oliva B., Alvarez-Vallina L. (2009). In vivo tumor targeting and imaging with engineered trivalent antibody fragments containing collagen-derived sequences. PLoS One.
4 Sanchez-Arevalo Lobo V.J., Cuesta A.M., Sanz L., Compte M., Garcia P., Prieto J., Blanco F.J., Alvarez-Vallina L. (2006). Enhanced antiangiogenic therapy with antibody-collagen XVIII NC1 domain fusion proteins engineered to exploit matrix remodeling events. Int J Cancer.
5 Gronwall C., Stahl S. (2009). Engineered affinity proteins--generation and applications. J Biotechnol.
6 Chames P., Baty D. (2009). Bispecific antibodies for cancer therapy. Curr Opin Drug Discov Devel.
7 Friedman M., Stahl S. (2009). Engineered affinity proteins for tumour-targeting applications. Biotechnol Appl Biochem.
8 Ortega N., Werb Z. (2002). New functional roles for non-collagenous domains of basement membrane collagens. J Cell Sci.
9 Maatta M., Virtanen I., Burgeson R., Autio-Harmainen H. (2001). Comparative analysis of the distribution of laminin chains in the basement membranes in some malignant epithelial tumors: the alpha1 chain of laminin shows a selected expression pattern in human carcinomas. J Histochem Cytochem.
10 Wang J., Hoshijima M., Lam J., Zhou Z., Jokiel A., Dalton N.D., Hultenby K., Ruiz-Lozano P., Ross J., Tryggvason K., Chien K.R. (2006). Cardiomyopathy associated with microcirculation dysfunction in laminin alpha4 chain-deficient mice. J Biol Chem.
11 Thyboll J., Kortesmaa J., Cao R., Soininen R., Wang L., Iivanainen A., Sorokin L., Risling M., Cao Y., Tryggvason K. (2002). Deletion of the laminin alpha4 chain leads to impaired microvessel maturation. Mol Cell Biol.
12 Ljubimova J.Y., Fujita M., Khazenzon N.M., Ljubimov A.V., Black K.L. (2006). Changes in laminin isoforms associated with brain tumor invasion and angiogenesis. Front Biosci.
13 Fujita M., Khazenzon N.M., Bose S., Sekiguchi K., Sasaki T., Carter W.G., Ljubimov A.V., Black K.L., Ljubimova J.Y. (2005). Overexpression of beta1-chain-containing laminins in capillary basement membranes of human breast cancer and its metastases. Breast Cancer Res.
14 Ljubimova J.Y., Fugita M., Khazenzon N.M., Das A., Pikul B.B., Newman D., Sekiguchi K., Sorokin L.M., Sasaki T., Black K.L. (2004). Association between laminin-8 and glial tumor grade, recurrence, and patient survival. Cancer.
15 Tran M., Rousselle P., Nokelainen P., Tallapragada S., Nguyen N.T., Fincher E.F., Marinkovich M.P. (2008). Targeting a tumor-specific laminin domain critical for human carcinogenesis. Cancer Res.
16 Sanz L., Kristensen P., Blanco B., Facteau S., Russell S.J., Winter G., Alvarez-Vallina L. (2002). Single-chain antibody-based gene therapy: inhibition of tumor growth by in situ production of phage-derived human antibody fragments blocking functionally active sites of cell-associated matrices. Gene Ther.